# Al^18^F-1,4,7-Triazacyclononane-1,4,7-diacetic acid-8-aminooctanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_

Chemical name: | Al^18^F-1,4,7-Triazacyclononane-1,4,7-diacetic acid-8-aminooctanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_
Abbreviated name: | Al^18^F-NOTA-8-Aoc-BBN[7-14]NH_2_
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRPR)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) for more information about gastrin-releasing peptide receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA)]

The amphibian bombesin (BBN or BN, a peptide of 14 amino acids) is an analog of human gastrin-releasing peptide (GRP, a peptide of 27 amino acids) that binds to GRP receptors (GRPR) with high affinity and specificity (1, 2). Both GRP and BBN share an amidated C-terminus sequence homology of seven amino acids, Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BBN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system and the gastrointestinal system. They also act as potential growth factors for both normal and neoplastic tissues (3). Specific BBN receptors (BBN-R) have been identified on central nervous system and gastrointestinal tissues and on a number of tumor cell lines (4). The BBN-R superfamily includes at least four different subtypes, namely the GRPR subtype (BB2), the neuromedin B (NMB) receptor subtype (BB1), the BB3 subtype, and the BB4 subtype. The findings of GRPR overexpression in various human tumors, such as breast, prostate, lung, colon, ovarian, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the GRPR (5, 6).

Various BBN analogs have been labeled with ^99m^Tc and ^111^In for single-photon emission computed tomography imaging studies (7) and with ^64^Cu, ^68^Ga, and ^86^Y for positron emission tomography imaging (PET) studies (8, 9). Dijkgraaf et al. (10) used 1,4,7-triazacyclononane-1,4-7-triacetic acid (NOTA) as a bifunctional chelator for labeling 8-aminooctanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_ (8-Aoc-BBN[7-14]NH_2_) with Al^18^F. Al^18^F-NOTA-8-Aoc-BBN[7-14]NH_2_ was evaluated as a PET imaging agent of GRPR in nude mice bearing human PC-3 prostate cancer cells.

### Related Resource Links:

- Chapters in MICAD (GRPR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=(GRPR%20OR%20GRP-R)%20+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), bombesin (http://www.ncbi.nlm.nih.gov/books?term=bombesin%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (GRPR (http://www.ncbi.nlm.nih.gov/gene/2925), GRP (http://www.ncbi.nlm.nih.gov/gene/2922))
- Articles in Online Mendelian Inheritance in Man (OMIM) (GRPR (http://www.ncbi.nlm.nih.gov/omim/305670), GRP (http://omim.org/entry/137260))
- Clinical trials (GRPR (http://www.clinicaltrials.gov/ct2/results?term=bombesin))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA+synthesis)]

8-Aoc-BBN[7-14]NH_2_ was prepared with solid-phase peptide synthesis, with the subsequent addition of a NOTA group to form NOTA-8-Aoc-BBN[7-14]NH_2_ (10). Al^18^F was added to a solution of NOTA-8-Aoc-BBN[7-14]NH_2_ in sodium acetate buffer (pH 4.1). The mixture was heated for 15 min at 100°C. The product, Al^18^F-NOTA-8-Aoc-BBN[7-14]NH_2_, was purified with high-performance liquid chromatography, with 50%–90% yield and a radiochemical purity of >95%. The specific activity of Al^18^F-NOTA-8-Aoc-BBN[7-14]NH_2_ was >10 MBq/nmol (0.27 mCi/nmol) at the end of synthesis. Total preparation time was ~45 min. Al^18^F-NOTA-8-Aoc-BBN[7-14]NH_2_ exhibited a Log P value of −1.47 ± 0.05.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA+in+vitro)]

Dijkgraaf et al. (10) performed in vitro inhibition studies of NOTA-8-Aoc-BBN[7-14]NH_2_ and Al^nat^F-NOTA-8-Aoc-BBN[7-14]NH_2_ in cultured human prostate PC-3 tumor cells with ^111^In-NOTA-8-Aoc-BBN[7-14]NH_2_. The 50% inhibition concentration (IC_50_) values for NOTA-8-Aoc-BBN[7-14]NH_2_ and Al^nat^F-NOTA-8-Aoc-BBN[7-14]NH_2_ were 0.37 ± 0.15 nM and 0.28 ± 0.15 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA+%20rodentia)]

Dijkgraaf et al. (10) performed ex vivo biodistribution studies of Al^18^F-NOTA-8-Aoc-BBN[7-14]NH_2_ (~0.3 nmol) in nude mice bearing PC-3 xenografts with (n = 5) or without (n = 2) coinjection of 100-fold excess unlabeled NOTA-8-Aoc-BBN[7-14]NH_2_ at 1 h after injection. Tumor accumulation was 2.15 ± 0.55% injected dose per gram (ID/g). The organ with the highest accumulation was the pancreas (27% ID/g), followed by the colon (3% ID/g), small intestine (2% ID/g), liver (1% ID/g), kidney (1% ID/g), stomach (1% ID/g), and lung (0.5% ID/g). Little accumulation was observed in the spleen, blood, and muscle (<0.5% ID/g). NOTA-8-Aoc-BBN[7-14]NH_2_ blocked tumor accumulation by 80%. Significant inhibition (>90%) was also observed in the pancreas, stomach, and colon. PET imaging in nude mice bearing PC-3 xenografts was performed with 2 MBq (0.05 mCi) Al^18^F-NOTA-8-Aoc-BBN[7-14]NH_2_ at 1 h after injection. The tumors were clearly visualized. High radioactivity was detected in the pancreas, with lesser amount in the liver and intestines. Co-injection of unlabeled peptide inhibited the visualization of the tumor and pancreas.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA+human)]

No publication is currently available.

## References

1 Gonzalez N., Moody T.W., Igarashi H., Ito T., Jensen R.T. (2008). Bombesin-related peptides and their receptors: recent advances in their role in physiology and disease states. Curr Opin Endocrinol Diabetes Obes.
2 Bertaccini G. (1976). Active polypeptides of nonmammalian origin. Pharmacol Rev.
3 Chung D.H., Evers B.M., Beauchamp R.D., Upp J.R., Rajaraman S., Townsend C.M., Thompson J.C. (1992). Bombesin stimulates growth of human gastrinoma. Surgery.
4 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
5 Reubi J.C., Wenger S., Schmuckli-Maurer J., Schaer J.C., Gugger M. (2002). Bombesin receptor subtypes in human cancers: detection with the universal radioligand (125)I-[D-TYR(6), beta-ALA(11), PHE(13), NLE(14)] bombesin(6-14). Clin Cancer Res.
6 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
7 Varvarigou A., Bouziotis P., Zikos C., Scopinaro F., De Vincentis G. (2004). Gastrin-releasing peptide (GRP) analogues for cancer imaging. Cancer Biother Radiopharm.
8 Biddlecombe G.B., Rogers B.E., de Visser M., Parry J.J., de Jong M., Erion J.L., Lewis J.S. (2007). Molecular imaging of gastrin-releasing peptide receptor-positive tumors in mice using 64Cu- and 86Y-DOTA-(Pro1,Tyr4)-bombesin(1-14). Bioconjug Chem.
9 Schuhmacher J., Zhang H., Doll J., Macke H.R., Matys R., Hauser H., Henze M., Haberkorn U., Eisenhut M. (2005). GRP receptor-targeted PET of a rat pancreas carcinoma xenograft in nude mice with a 68Ga-labeled bombesin(6-14) analog. J Nucl Med.
10 Dijkgraaf I., Franssen G.M., McBride W.J., D'Souza C.A., Laverman P., Smith C.J., Goldenberg D.M., Oyen W.J., Boerman O.C. (2012). PET of Tumors Expressing Gastrin-Releasing Peptide Receptor with an 18F-Labeled Bombesin Analog. J Nucl Med.